# Air-filled, cross-linked, human serum albumin microcapsules

Chemical name: | Air-filled, cross-linked human serum albumin microcapsules
Abbreviated name: | Air-filled HAS microcapsules
Synonym: | Quantison^TM^
Agent Category: | Albumin
Target: | Non-targeted contrast agent, blood pool
Target Category: | Passive nontargeted filling of cardiac chambers
Method of detection: | Ultrasound (US)
Source of signal/contrast: | Air-filled microbubble
Activation: | No
Studies: | - In vitro; - Humans

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28air%20filled%20human%20serum%20albumin%20microcapsules%29%20OR%20quantison)]

The air-filled, cross-linked, human serum albumin (HSA) microcapsules (air-filled HSA microcapsules) is a stabilized mirobubble formulation that is being developed as an ultrasound (US) contrast agent for use in echocardiography to enhance US images (1)

US contrast agents, or echopharmaceuticals, are designed to change the attenuation (absorption, reflection, and refraction) or impedance (resistance to sound propagation) of sound to enhance the differentiation of the signal (echo) of a target organ from that of the surrounding tissue (2-5). Gas-liquid emulsions (i.e., microbubbles or gaseous particles) are highly echogenic in vivo because of the nonlinear rarefaction and compression effects that lead to volume pulsations of microbubbles (3, 6, 7). HSA, synthetic polymers, and phospholipids have been used to construct the membranes of these bubbles. Microbubble preparations of various formulations have been developed, and their clinical usefulness depends very much on the size and stability of these bubbles in vivo. The current clinical application of these agents is in myocardial contrast echocardiography (MCE) (8).

In addition to acoustic parameters, microbubble preparations must meet two other requirements in order to be useful for MCE applications. Microtubble preparations cannot be trapped significantly by the lung capillaries and they must be able to survive the high intracardiac pressure. Air-filled microbubbles stabilized within a galactose matrix were the first commercially available echopharmaceutical (9). However, these microbubbles are not stable enough to pass through the pulmonary capillary bed after a peripheral intravenous injection and can be used only to opacify the right heart chamber. Sonicated human serum microspheres (Sonicated HSM) were the first US contrast agent approved in the United States for cardiac applications. HSM consists of air-filled microbubbles stabilized in a thin shell of HSA with a mean diameter of 3.8 ± 2.5 μm (10). Although these air-filled microbubbles are very sensitive to pressure changes with an in vivo half-life (t_½_) of <1 min, they can pass through the pulmonary capillary bed and reach the left heart chamber. The in vivo life-times of air-filled microbubbles can be prolonged by increasing the stiffness of the bubble shell (11). Air-filled HSA microcapsules have stabilized shells that can withstand pressures in excess of 300 mm Hg (1). Other microbubble preparations use perfluorocarbons which dissolve poorly in blood to increase the stability of the microbubbles (12).

Serious cardiopulmonary reactions following the administration of ultrasound microbubble contrast agents have been reported (13). In 2007, the US FDA (http://www.fda.gov/cder/drug/InfoSheets/HCP/microbubbleHCP.htm) requested that warnings emphasizing the risk for serious cardiopulmonary reactions be added to the labeling of these agents. The uses of these agents are contraindicated in patients with unstable cardiopulmonary status.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28air%20filled%20human%20serum%20albumin%20microcapsules%29%20OR%20quantison%29%20AND%20synthesis)]

Air-filled HSA microcapsules are air bubbles encapsulated by a shell of HSA (1, 11). The microbubble shell is formed by spray-drying a solution of HSA. This shell is stabilized by heat fixation and chemical cross-linking. The final preparation is a dry powder that must be resuspended before use. The mean diameter is 3.2 μm, and less than 0.5% of the preparation had a diameter >6 μm. The shell thickness is 200-300 nm and is able to withstand static pressure up to 600 mm Hg without losing the air within the microbubble. The density of the bubbles is approximately 780 kg/m^3^. The particle density in the preparation is about 1.5 х 10^9^ bubbles per ml.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28air%20filled%20human%20serum%20albumin%20microcapsules%29%20OR%20quantison%29%20AND%20in%20vitro)]

Chatterjee and Sarkar (14) suggested an interfacial rheological model with intrinsic surface rheology for studying the US microbubbles. Frinking and De Jong (11) studied the in vitro scatter and attenuation properties of air-filled HSA microcapsules based on an adapted version of the Rayleigh-Plesset equation which treats the microbubbles as a viscoelastic solid. The acoustic transmission and scattering were measured in the frequency band from 1-10 MHz. The effective bulk modulus (elasticity) of air-filled HSA microcapsules was 17.4 MPa and independent of the bubble diameter. In comparison, the effective bulk modulus of sonicated HSM was 1.3 MPa and increased for decreasing bubble diameter. The acoustic efficiency of air-filled HSA microcapsules was relatively low for low acoustic pressures but the measured scattering coefficient abruptly increased above an acoustic pressure of 200 kPa.

Moran et al. (15) used an in vitro tissue-mimicking phantom to study the scatter phenomenon of air-filled HSA microcapsules. A 3.5-5.0 MHz probe was used. At high concentrations (no dilution), no significant change in mean integrated backscatter was observed during continuous sonication. For medium (1:25 dilution) and low (1:50 dilution) concentrations, mean integrated backscatter values reached their maximum values and then decreased.

In various experiments, Sboros et al. studied the in vitro properties of US contrast agents (16-20). Using dilute suspensions of microbubbles, air-filled HSA microcapsules appeared to produce an increasing number of scattering events per unit volume with increasing acoustic pressure. However, the behavior across the acoustic pressure range was not uniform. Free bubbles appeared at the high acoustic pressure of 0.83 MPa peak negative pressure. Postema et al. (21) investigated the phenomenon of sonic cracking. They used high-speed photography to observe the high-mechanical index US-induced air released from air-filled HSA microcapsules For air-filled HSA microcapsules, sonic cracking was observed more often at driving frequency closer to the resonance frequency (1.7 MHz). Most of the released air bubbles had smaller equilibrium diameters (between 1.25 and 1.75 μm).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28air%20filled%20human%20serum%20albumin%20microcapsules%29%20OR%20Quantison%29%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28air%20filled%20human%20serum%20albumin%20microcapsules%29%20OR%20Quantison%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28air%20filled%20human%20serum%20albumin%20microcapsules%29%20OR%20Quantison%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28air%20filled%20human%20serum%20albumin%20microcapsules%29%20OR%20Quantison%29%20AND%20human)]

Perkins et al. (1) used ^123^I-labeled, air-filled HSA microcapsules and gamma imaging to study the biodistribution of air-filled HSA microcapsules in 12 normal healthy male subjects. The chloramines-T method was used to perform radiolabeling radiolabeling. The radiolabeling efficiency was 15%. The preparation was washed four times so that 100% of the radioactivity was bound to the microcapsules. Each subject received a dose of 50 MBq (1.35 mCi) with a total of 50 million microcapsules/kg. All subjects also received 100 mg potassium iodide three times to reduce thyroid uptake of [^123^I]iodide. Gamma planar imaging showed immediate radioactivity uptake in the myocardium. There was evidence of myocardial perfusion at 3 min. The myocardial radioactivity which displayed a doughnut pattern, appeared to be more intense than that in the blood of the left ventricle. The washout of the agent from the myocardium was observed as no radioactivity was detected after 3 h. There was also rapid uptake of radioactivity by the liver and spleen. Posterior images showed some bone marrow uptake. Within the first hour, the liver had the highest radioactivity level of 41.8 ± 10.4% injected dose (ID). Transient lung activity of 4.0 ± 3.4% ID was observed. The maximum heart radioactivity level was 0.7 ± 0.4% ID at 0.06 hr. The spleen and kidneys had maximum radioactivity levels of 11.0 ± 6.2% ID at 1 hr and 1.6 ± 1.0% ID at 5 min, respectively. There was a rapid initial elimination of radioactivity from the blood with 15% ID at 5 min. About 63% ID radioactivity was excreted into the urine over 58 h and <0.5% in the feces over 36 h.

In a dose-finding study, van der Wouw et al. (22) conducted echocardiographic imaging (two-dimensional and color Doppler) in 12 healthy male volunteers. Each volunteer received two i.v. doses. The first dose was 25, 50, 100 or 150 х 10^6^ microcapsules/kg, and the second dose was 300 х 10^6^ microcapsules/kg. Air-filled HSA microcapsules required higher US output for visualization but the US contrast was visible in the left ventricular cavity for up to 30 min in two-dimensional and up to 60 min in color Doppler imaging.

## NIH Support

NIH P50 CA103130-01.

## References

1 Perkins A.C., Frier M., Hindle A.J., Blackshaw P.E., Bailey S.E., Hebden J.M., Middleton S.M., Wastie M.L. (1997). Human biodistribution of an ultrasound contrast agent (Quantison) by radiolabelling and gamma scintigraphy. Br J Radiol.
2 Morawski A.M., Lanza G.A., Wickline S.A. (2005). Targeted contrast agents for magnetic resonance imaging and ultrasound. Curr Opin Biotechnol.
3 Schutt E.G., Klein D.H., Mattrey R.M., Riess J.G. (2003). Injectable microbubbles as contrast agents for diagnostic ultrasound imaging: the key role of perfluorochemicals. Angew Chem Int Ed Engl.
4. Swanson, D.P., Enhancement agents for ultrasound: Fundamentals, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 682-687.
5. Gobuty, A.H., Perspectives in ultrasound contrast agents, in Contrast media: Biologic effects and clinical application, Z. Parvez, R. Moncada and M. Sovak, Editor. 1987, CRC: Boca Raton, Florida. p. 145-155.
6 Averkiou M., Powers J., Skyba D., Bruce M., Jensen S. (2003). Ultrasound contrast imaging research. Ultrasound Q.
7 Miller A.P., Nanda N.C. (2004). Contrast echocardiography: new agents. Ultrasound Med Biol.
8 Murthy T.H., Li P., Locvicchio E., Baisch C., Dairywala I., Armstrong W.F., Vannan M. (2001). Real-time myocardial blood flow imaging in normal human beings with the use of myocardial contrast echocardiography. J Am Soc Echocardiogr.
9 Correas J.M., Bridal L., Lesavre A., Mejean A., Claudon M., Helenon O. (2001). Ultrasound contrast agents: properties, principles of action, tolerance, and artifacts. Eur Radiol.
10. Summary of safety and effectiveness of Albunex. PMA number P9000059/Supplement 004, Mallinckrodt, Inc. p. 1-28.
11 Frinking P.J., de Jong N. (1998). Acoustic modeling of shell-encapsulated gas bubbles. Ultrasound Med Biol.
12 Mattrey R.F. (1990). Sonographic enhancement of Doppler signals and perfused tissues with perfluorooctylbromide. Invest Radiol.
13 Blomley M., Claudon M., Cosgrove D. (2007). WFUMB Safety Symposium on Ultrasound Contrast Agents: clinical applications and safety concerns. Ultrasound Med Biol.
14 Chatterjee D., Sarkar K. (2003). A Newtonian rheological model for the interface of microbubble contrast agents. Ultrasound Med Biol.
15 Moran C.M., Anderson T., Sboros V., Sutherland G.R., Wright R., McDicken W.N. (1998). Quantification of the enhanced backscatter phenomenon from an intravenous and an intra-arterial contrast agent. Ultrasound Med Biol.
16 Sboros V., Moran C.M., Anderson T., Gatzoulis L., Criton A., Averkiou M., Pye S.D., McDicken W.N. (2001). An in vitro system for the study of ultrasound contrast agents using a commercial imaging system. Phys Med Biol.
17 Sboros V., Moran C.M., Pye S.D., McDicken W.N. (2001). Contrast agent stability: a continuous B-mode imaging approach. Ultrasound Med Biol.
18. Sboros, V., C.A. MacDonald, S.D. Pye, C.M. Moran, J. Gomatam, and W.N. McDicken, The dependence of ultrasound contrast agents backscatter on acoustic pressure: theory versus experiment. Ultrasonics, 2002. 40(1-8): p. 579-83.
19 Sboros V., Moran C.M., Pye S.D., McDicken W.N. (2003). The behaviour of individual contrast agent microbubbles. Ultrasound Med Biol.
20 Sboros V., Ramnarine K.V., Moran C.M., Pye S.D., McDicken W.N. (2002). Understanding the limitations of ultrasonic backscatter measurements from microbubble populations. Phys Med Biol.
21 Postema M., Bouakaz A., Versluis M., de Jong N. (2005). Ultrasound-induced gas release from contrast agent microbubbles. IEEE Trans Ultrason Ferroelectr Freq Control.
22 van der Wouw P.A. Braune A.C. Levi M. Bailey S.E. Quantison, a new long-living ultrasound contrast agent: experience in human volunteers J Am Coll Cardiol 1997 29Suppl A299A